# Biotinylated bovine serum albumin linked to gadolinium diethylenetriaminepentaacetic acid

Chemical name: | Biotinylated bovine serum albumin linked to gadolinium diethylenetriamine pentaacetic acid
Abbreviated name: | Biotin-BSA-GdDTPA
Synonym:
Agent Category: | Protein
Target: | Tumor-associated stroma
Target Category: | Uptake
Method of detection: | Magnetic resonance imaging (MRI)
Source of Signal/Contrast: | Gadolinium
Activation: | No
Studies: | - In vitro; - Rodents | No structure information is available.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=biotin+BSA+GdDTPA+FAM)]

An interaction between the epithelium and the surrounding stromal tissue that are separated by a basement membrane is responsible for maintenance of the epithelial tissue. Also, the stroma contains fibroblasts, leukocytes, and epithelial cells that are embedded in an extracellular matrix. Development of an epithelial carcinoma caused by a transformation of the epithelium results in stromal changes that involve the fibroblastic stroma and are considered essential for progression of the solid cancerous tumors (1-3). The fibroblasts in the stroma are believed to differentiate into myofibroblasts that have contractile properties and characteristically produce α-smooth muscle actin (α-SMA). The myofibroblasts have been shown to participate in tumor angiogenesis that is considered essential for maintenance and progression of the cancer (1, 4-6). The myofibroblasts in turn differentiate into pericyte-like cells, and there is evidence suggesting that these cells play an important function in angiogenesis (7). Because several cell types are involved in the angiogenic process, the exact interaction between the various cell types, particularly the endothelial cells, the fibroblasts, and the myofibroblasts, is unclear. Granot et al. suggested that in vivo monitoring of the different cell types may reveal the function of each cell type in the tumor angiogenesis process (8).

The technique of magnetic resonance imaging (MRI) with the use of ferromagnetic or fluorinated nanoparticles has been used successfully to investigate cell dynamics in an in vivo setting (9, 10). Granot et al. used a similar approach to study the migration of fibroblasts after labeling them with biotinylated bovine serum albumin linked to gadolinium diethylenetriamine pentaacetate (biotin-BSA-GdDTPA) (8). Biotin-BSA-GdDTPA was also labeled with 5(6)-carboxyfluorescein succinimidyl ester (biotin-BSA-GdDTPA-FAM) to study uptake of the contrast agent (CA) by the myofibroblasts (8). Biotinylated BSA was used to facilitate labeling with avidin-conjugated 5(6)fluorescein isothiocyanate-mixed isomer (FITC) to study the biodistribution of biotin-BSA-GdDTPA in nude mice bearing fibroblast cell xenograft tumors in the hind limbs.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=biotin+BSA+GdDTPA+synthesis)]

The synthesis of biotin-BSA-GdDTPA and biotin-BSA-GdDTPA-FAM has been described elsewhere (11, 12). One to two biotin moieties and 27 GdDTPA moieties were reported to be bound to each BSA molecule (8).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=biotin+BSA+GdDTPA+in+vitro)]

To investigate possible internalization of biotin-BSA-GdDTPA by tumor cells, cells derived from MLS cell (of human ovarian carcinoma origin) xenograft tumors in nude mice and normal human breast fibroblasts which were exposed to biotin-BSA-GdDTPA under ex vivo conditions (8). Confocal fluorescence microscopy of the labeled tumors or fibroblasts showed that the CA was internalized by the cells. Localization of the CA to the myofibroblasts was confirmed with the use of an alkaline phosphate-conjugated anti–α-SMA monoclonal antibody. In addition, MRI of the cells showed an increase in the R_1_ relaxation rate of the labeled fibroblasts in culture that remained high for at least 2 weeks; this rate also increased on cell proliferation, indicating retention, intracellular processing, and redistribution of the CA in the cells. In another study, exposure of the cells to nystatin (that inhibits caveolae-mediated endocytosis) was shown to significantly (P = 0.006) reduce uptake of biotin-BSA-GdDTPA by the cells, indicating that endocytosis and caveolae have a role in internalization of the CA (8, 13).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=biotin+BSA+GdDTPA+rodentia)]

Xenograft tumors were generated in hind limbs of CD-1 nude mice (n = 4 animals) by the co-injection of MLS (a human ovarian carcinoma cell line) and PF42T (human tumor–derived fibroblasts) cells (8). Biotin-BSA-GdDTPA was administered to these animals through the tail vein, and animals were euthanized after 30 min. To investigate CA distribution in the tumor mass, the tumors were retrieved from the animals and tumor histological sections were stained with avidin-FITC. Fluorescence microscopy revealed that the CA was present in a specific pattern associated with stromal cell tracks in the histological sections.

To investigate the in vivo visibility of cells labeled with biotin-BSA-GdDTPA, CD-1 nude mice were co-injected with MLS and cos-7 cells pre-labeled ex vivo with CA (n = 4 animals) or without CA (controls; n = 4 animals) (8). One day after the injection, MRI was performed on the animals, and a significantly higher (P = 0.01) R_1_ value, compared to the control animal tumors, was obtained from tumors of the CA-treated cells indicating the cells migrated to the stroma and facilitated spread of the cancer.

From these studies the investigators concluded that biotin-BSA-GdDTPA can be used for in vivo tracking of cells using MRI.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Biotinylated+BSA+Gd+DTPA+Non+Human+Primates)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Biotinylated+BSA+Gd+DTPA+Human+Studies)]

No references are currently available.

## Supplemental Information

[Disclaimers]

## NIH Support

Some studies in this chapter were funded by National Institutes of Health grants RO1 CA75334 and RO1 CA90471.

## References

1 De Wever O., Mareel M. (2003). Role of tissue stroma in cancer cell invasion. J Pathol.
2 Kunz-Schughart L.A., Knuechel R. (2002). Tumor-associated fibroblasts (part II): Functional impact on tumor tissue. Histol Histopathol.
3 Kunz-Schughart L.A., Knuechel R. (2002). Tumor-associated fibroblasts (part I): Active stromal participants in tumor development and progression?. Histol Histopathol.
4 Elenbaas B., Weinberg R.A. (2001). Heterotypic signaling between epithelial tumor cells and fibroblasts in carcinoma formation. Exp Cell Res.
5 Walter-Yohrling J., Pratt B.M., Ledbetter S., Teicher B.A. (2003). Myofibroblasts enable invasion of endothelial cells into three-dimensional tumor cell clusters: a novel in vitro tumor model. Cancer Chemother Pharmacol.
6 Gilead A., Meir G., Neeman M. (2004). The role of angiogenesis, vascular maturation, regression and stroma infiltration in dormancy and growth of implanted MLS ovarian carcinoma spheroids. Int J Cancer.
7 Betsholtz C., Lindblom P., Gerhardt H. (2005). Role of pericytes in vascular morphogenesis. Exs.
8 Granot D., Kunz-Schughart L.A., Neeman M. (2005). Labeling fibroblasts with biotin-BSA-GdDTPA-FAM for tracking of tumor-associated stroma by fluorescence and MR imaging. Magn Reson Med.
9 Ruiz-Cabello J., Walczak P., Kedziorek D.A., Chacko V.P., Schmieder A.H., Wickline S.A., Lanza G.M., Bulte J.W. (2008). In vivo "hot spot" MR imaging of neural stem cells using fluorinated nanoparticles. Magn Reson Med.
10 Focke A., Schwarz S., Foerschler A., Scheibe J., Milosevic J., Zimmer C., Schwarz J. (2008). Labeling of human neural precursor cells using ferromagnetic nanoparticles. Magn Reson Med.
11 Dafni H., Israely T., Bhujwalla Z.M., Benjamin L.E., Neeman M. (2002). Overexpression of vascular endothelial growth factor 165 drives peritumor interstitial convection and induces lymphatic drain: magnetic resonance imaging, confocal microscopy, and histological tracking of triple-labeled albumin. Cancer Res.
12 Dafni H., Landsman L., Schechter B., Kohen F., Neeman M. (2002). MRI and fluorescence microscopy of the acute vascular response to VEGF165: vasodilation, hyper-permeability and lymphatic uptake, followed by rapid inactivation of the growth factor. NMR Biomed.
13 Razani B., Woodman S.E., Lisanti M.P. (2002). Caveolae: from cell biology to animal physiology. Pharmacol Rev.